# ^125^I-Hydroxylated-single-walled nanotubes

Chemical name: | ^125^I-Hydroxylated-single-walled nanotubes
Abbreviated name: | ^125^I-SWNTols
Synonym:
Agent category: | Nanoparticle
Target: | Non-targeted
Target category: | Other
Method of detection: | SPECT, planar gamma imaging
Source of signal\contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=SWNT)]

Optical fluorescence imaging is increasingly used to visualize biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Carbon nanotubes are made of C_60_ fullerene carbon units, which respond to local dielectric changes without photobleaching (3, 4). They can be tuned in a range of wavelengths for NIR absorption, thus providing broad excitation profiles and high absorption coefficients. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds for in vitro and in vivo studies (5). Single-walled carbon nanotubes (SWNTs) have a diameter of 1–5 nm and a length of 300–1,000 nm, and they have been shown to be non-toxic to cells in vitro. However, there have been limited in vivo studies of SWNT toxicological and pharmacological profiles in small animals. SWNTs have been hydroxylated with KOH and radiolabeled with Na^125^I to form ^125^I-hydroxylated-single-walled nanotubes (^125^I-SWNTols) for biodistribution studies in mice (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+synthesis)]

Wang et al. (6) performed hydroxylation of SWNTs by incubating SWNTs (1.4 nm in diameter, 340 nm in length) with KOH for 1 h at room temperature. Hydroxylated SWNTs (SWNTols) were isolated with size-exclusion column chromatography. SWNTols were iodinated with Na^125^I by the chloramine-T method for 5 min at room temperature. ^125^I-SWNTols were isolated with column chromatography with a radiochemical purity of >96%. There are only five ^125^I atoms per 100 SWNTols. SWNTols were estimated to have a molecular weight of >500,000 Da. No dissociation of ^125^I ions from solutions of ^125^I-SWNTols was observed at 11 days after labeling. Photoelectron spectroscopic measurement confirmed the presence of the C-I covalent bonds in ^125^I-SWNTols.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+in+vitro)]

Yehia et al. (7) performed transmission electron microscopy (TEM) and confocal Raman spectroscopy using human HeLa cells after incubation with SWNTs for up to 60 h at 37°C. SWNTs were taken up by HeLa cells in a time-dependent manner with confocal Raman spectroscopy. TEM revealed that SWNTs were in intracellular vacuoles but not in the nucleus. SWNTs did not affect the growth rates of HeLa cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+%20rodentia)]

Wang et al. (6) studied long-term biodistribution in normal mice (n = 5/group) up to 18 days after intraperitoneal injection of 1.5 µg ^125^I-SWNTols/mouse. Accumulation of ^125^I-SWNTols was low in macrophages in the liver (<20 ng/g) and spleen (<20 ng/g) from 1–24 h, and it was almost undetectable by 72 h. ^125^I-SWNTols were not detected in the blood after 72 h. The organs with the highest accumulation of ^125^I-SWNTols at 6 h were the stomach, (~100 ng/g), bone (~100 ng/g), and kidney (~100 ng/g) with gradual clearance to background levels by 6 d. The liver, lung, and spleen accumulated <25 ng/g. Little accumulation was observed in the muscle and brain. Most of the ^125^I-SWNTols (>75%) were found in the urine 11 days after injection. No physiological complications were observed in the mice at 18 days. Similar distribution patterns were observed at 3 h with intraperitoneal injection, intravenous injection, gavage, and subcutaneous injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Indium+SWNT+human)]

No publication is currently available.

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hersam M.C. (2008). Progress towards monodisperse single-walled carbon nanotubes. Nat Nanotechnol.
4 Barone P.W., Baik S., Heller D.A., Strano M.S. (2005). Near-infrared optical sensors based on single-walled carbon nanotubes. Nat Mater.
5 Klumpp C., Kostarelos K., Prato M., Bianco A. (2006). Functionalized carbon nanotubes as emerging nanovectors for the delivery of therapeutics. Biochim Biophys Acta.
6 Wang H., Wang J., Deng X., Sun H., Shi Z., Gu Z., Liu Y., Zhao Y. (2004). Biodistribution of carbon single-wall carbon nanotubes in mice. J Nanosci Nanotechnol.
7 Yehia H.N., Draper R.K., Mikoryak C., Walker E.K., Bajaj P., Musselman I.H., Daigrepont M.C., Dieckmann G.R., Pantano P. (2007). Single-walled carbon nanotube interactions with HeLa cells. J Nanobiotechnology.